# Pamidronate-IRDye78

Chemical name: | Pamidronate-IRDye78
Abbreviated name: | Pam78
Synonym:
Agent category: | Compound
Target: | Hydroxyapatite
Target category: | Acceptor
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal\contrast: | IRDye78
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Pam78%5BAll%20Fields%5D%20OR%20IRDye78%5BAll%20Fields%5D)]

Optical fluorescence imaging is increasingly used to obtain biological functions of specific targets in vitro and in small animals (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when visible light (350-700 nm) absorbing fluorophores are used because of high tissue absorption and scatter. Near-infrared (NIR) fluorescence (700-900 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared to visible fluorescence detection. They also have high sensitivity resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region was also compatible with solid-state optical components such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alterative to radionuclide imaging in vitro and in small animals.

IRDye78 is a heptamethine indocyanine-type NIR fluorophore with peak absorption at 771 nm, and peak excitation emission at 806 nm. It provides a quantum yield of 14.2%. It has a molecular weight of 1083 Da. IRDye78 is a highly charged IR-786 derivative, which localized to mitochondria at low concentrations and endoplasmic reticulum (ER) at high concentrations in vitro (3). IRDye78 was shown to be a useful perfusion agent in myocardium. IRDye78 N-hydroxysuccinimide (NHS) ester can be conjugated to antibodies and low-molecular weight ligands with one or more free primary amines.

Osteoblasts (mineralization) and osteoclasts (demineralization) are two importance cell types in development and integrity of vertebral skeleton (4, 5). Osteoblast-like cells are present in vascular tissues and play a role in arteriosclerosis (6). Microcalcifications are found in breast tissue (7, 8). Hydroxyapatite (HA) is a mineral product deposited in the bone and vascular tissue by the osteoblast. HA binds pyrophosphates and phosphonates with high affinity. Nitrogen-containing synthetic diphosphonates are inhibitors of farnesyl diphosphate synthase (FDPS) of osteoclast and are used for treatment of osteoporosis (bone resorption) (9). Inhibition of FDPS inhibits osteoclast bone-resorption activity and induces osteoclast apoptosis (10, 11). Diphosphonates bind to bone mineral with high affinity for their long duration of action. For example, [^99m^Tc]Methylene diphosphonate (MDP) was developed for bone scanning (12) and it is believed that it binds to HA. Pamidronate (Pam) is a diphosphonate derivative with a single primary amine for conjugation with IRDye78-NHS ester to form Pam78. Pam78 exhibits rapid and specific binding to HA in vitro and in vivo. Zaheer et al. (13) demonstrated NIR fluorescence detection of bone with Pam78 in nude mice. A simple and rapid rat model of focal calcification in breast cancer tumors was validated by Pam78 NIR imaging (14).

### Related Resource Links:

- Chapters in MICAD (Diphosphonate (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=diphosphonate+AND+micad%5Bbook%5D))
- Gene information in NCBI (Farnesyl diphosphate synthase (http://www.ncbi.nlm.nih.gov/gene/2224))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Farnesyl diphosphate synthase (http://omim.org/entry/134629?search=Farnesyl%20diphosphate%20synthase&highlight=diphosphate%20farnesyl%20synthase))
- Clinical trials (Pamidronate (http://www.clinicaltrials.gov/ct2/results?term=Pamidronate))
- Drug information in FDA (Pamidronate (http://google2.fda.gov/search?q=Pamidronate&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Pam78%5BAll%20Fields%5D%20OR%20IRDye78%5BAll%20Fields%5D)]

IRDye78 monofunctional NHS ester reacted with the single primary amino group of Pam to form Pam78, which was purified using thin-layer chromatography and confirmed by mass spectroscopy. Pam78 had peak absorption at 771 nm and peak emission at 796 nm. The conjugation yields were 18-21% (13).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Pam78%5BAll%20Fields%5D%20AND%20%22in%20vitro%22%5BAll%20fields%5D)]

In a kinetic binding assay, Pam78 (5 μM) exhibited rapid binding to 1.5 mM HA, with 37% binding capacity achieved in 5 min and a start to plateau by 1 h. A similar concentration of IRDye78 showed no detectable binding to HA. Pam78 binding to HA was inhibited by Pam with an IC_90_ of 800 μM. HA was estimated to have a maximum binding capacity of 0.84 mmol of Pam78 per gram of HA (13).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Pam78%5BAll%20Fields%5D%20AND%20rodentia)]

Nude mice received injections intravenously with 2.6 nmol of Pam78 or IRDye78. Peak serum concentration of 2.6 μM was reached within 1 min for both. IRDye78 exhibited a two-phase elimination from the plasma, with early and late half-lives of 7.2 and 24.7 min, respectively (3). Pam78 also showed a faster two-phase elimination, having early and late half-lives of 5.0 and 15.4 min, respectively (13).

NIR fluorescence reflectance imaging showed negligible autofluorescence of the mice. IRDye78 fluorescence was homogeneous in the entire mouse within 1 min and stable for the next 15 min (13). The dye was eliminated to near background by the urinary and biliary systems over the next 6 h. Pam78 showed a similar rapid distribution. However, Pam78 uptake in the spine, ribs, paws, and knees could be detected as early as 15 min. By 3 h, most bony structures were visible. At 6 h, most of the bones of the mouse could be visualized by high-resolution imaging. However, deep bone structures were either poorly visualized or not visualized at all as a result of skin and soft-tissue attenuation and scatter. MRI T1-weighted scans were used to measure the distance between the skin surface and the target bone. An estimation of intensity attenuation was 32% as compared with 44% obtained by actual NIR measurements with and without skin. Optical scatter is a major limitation to NIR planar imaging. There was a 57% uptake of Pam78 in the ribs as compared with 52% uptake of ^99m^Tc-MDP.

Female rats were implanted with the R3230 mammary adenocarcinoma cell line in the mammary fat pad. After growth to 1-2 cm in diameter, tumors were implanted with 100 μM HA crystals (positive control) or calcium oxalate crystals (negative control). Twenty-four hours after crystal implantation, rats were injected intravenously with Pam78 (0.1 μmol/kg), and the tumors were imaged using a reflectance optical imaging system. Tumors implanted with HA crystals displayed bright, focal, NIR fluorescence in the area of crystal implantation. Control tumors, grown in the same animal and implanted with calcium oxalate, did not display any NIR fluorescence. A simple and rapid animal model of focal calcification in breast cancer tumors was validated by a NIR fluorescent agent specific for HA (14).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Pam78%5BAll%20Fields%5D%20AND%20%28animals%20NOT%20rodentia%20NOT%20primate%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Pam78%5BAll%20Fields%5D%20AND%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Pam78%5BAll%20Fields%5D%20AND%20human)]

No publication is currently available.

## NIH Support

R21 CA88245, R21 CA88870, CA70362

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Nakayama A., del Monte F., Hajjar R.J., Frangioni J.V. (2002). Functional near-infrared fluorescence imaging for cardiac surgery and targeted gene therapy. Mol Imaging.
4 Marks S.C., Popoff S.N. (1988). Bone cell biology: the regulation of development, structure, and function in the skeleton. Am J Anat.
5 Seibel M.J. (2004). Bone metabolism, mineral homeostasis and its pharmacological modulation. Clin Lab.
6 Demer L.L., Tintut Y. (2003). Mineral exploration: search for the mechanism of vascular calcification and beyond: the 2003 Jeffrey M. Hoeg Award lecture. Arterioscler Thromb Vasc Biol.
7 Bassett L.W. (1992). Mammographic analysis of calcifications. Radiol Clin North Am.
8 Bassett L.W. (2000). Digital and Computer-Aided Mammography. Breast J.
9 Body J.J. (2003). Rationale for the use of bisphosphonates in osteoblastic and osteolytic bone lesions. Breast.
10 Drake M.T., Clarke B.L., Khosla S. (2008). Bisphosphonates: mechanism of action and role in clinical practice. Mayo Clin Proc.
11 Russell R.G., Rogers M.J. (1999). Bisphosphonates: from the laboratory to the clinic and back again. Bone.
12 Subramanian G., McAfee J.G., Blair R.J., Kallfelz F.A., Thomas F.D. (1975). Technetium-99m-methylene diphosphonate--a superior agent for skeletal imaging: comparison with other technetium complexes. J Nucl Med.
13 Zaheer A., Lenkinski R.E., Mahmood A., Jones A.G., Cantley L.C., Frangioni J.V. (2001). In vivo near-infrared fluorescence imaging of osteoblastic activity. Nat Biotechnol.
14 Lenkinski R.E., Ahmed M., Zaheer A., Frangioni J.V., Goldberg S.N. (2003). Near-infrared fluorescence imaging of microcalcification in an animal model of breast cancer. Acad Radiol.